# ^111^In conjugated to benzyl-diethylenetriaminepentaacetic acid-human epidermal growth factor

Chemical name: | ^111^In conjugated to benzyl-diethylenetriaminepentaacetic acid-human epidermal growth factor
Abbreviated name: | [^111^In]Bz-DTPA-hEGF
Synonym:
Agent Category: | Receptor ligand
Target: | Epidermal growth factor receptor (EGFR)
Target Category: | Receptor
Method of detection: | Single-photon computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click here for the protein and nucleotide (http://www.ncbi.nlm.nih.gov/CCDS/CcdsBrowse.cgi?REQUEST=CCDS&GO=MainBrowse&DATA=CCDS3689.1) sequence of human EGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=glioblastoma+and+EGFR)]

Gliomas are the most common form of malignant brain tumors in humans. Although surgery, chemotherapy, or radiotherapy alone, or a combination of these therapies, comprise the most common treatment methods for this ailment, the prognosis for the patient is usually very poor (1). As an alternative, investigators have been exploring the use of receptor-based therapy for this cancer because with this technique the anti-cancer drugs can be targeted specifically to the tumor. Because the epidermal growth factor (EGF) receptor (EGFR) is known to be overexpressed in many glioma tumor types, it has been targeted for the treatment of this cancer with small-molecule drugs (SMDs) or antibodies (Abs) directed against the EGFR (click here for references: PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti+egfr+ligand+and+gliomas)). The EGFR is a membrane-bound receptor with an extracellular region that can bind several different ligands, and it mediates its activity through an intracellular tyrosine kinase (TK) signaling pathway. This receptor has been shown to have a major role in the pathogenesis and progression of different cancers, as detailed elsewhere (2, 3). When a ligand, including an anti-EGFR Ab, is bound to the EGFR, the TK signaling pathway is activated and the receptor-ligand complex is rapidly internalized by the cell (4). The phenomenon of receptor internalization has been used by some investigators in an effort to improve the detection or treatment for a disease, including cancers, by linking a toxin, a SMD, or a radionuclide to Abs directed to a specific receptor (5-7).

Dadparvar et al. used anti-EGFR Abs labeled with radioactive indium (^111^In, imaging gamma rays and Auger electrons emitter) to detect gliomas with scintigraphy in 23 human patients, and the investigators observed that uptake of the radiolabeled Ab by the tumors was variable (8). They concluded that uptake of the labeled Ab by the gliomas had almost no prognostic value even if the tumors were overexpressing the EGFR. This could be attributed to the large size of the Abs (~150 kDa), which may interfere with diffusion into deeper parts of the tumors. Because of its small size (~6 kDa), the use of radioiodinated (^131^I) EGF for the radiotherapy of malignant gliomas has also been investigated, but this radiolabeled ligand was not very effective because ^131^I dissociated quickly from the peptide and was excreted out of the cells (9). Subsequently, radioiodinated EGF-dextran (RED) conjugates were evaluated using human cultured glioma cell spheroids as a tumor model (10). Tumor penetration of the RED was reported to be slow, probably because of the large size of the radiolabeled peptide-dextran conjugate, and it took several hours for the radioactivity to penetrate into deeper parts of the spheroids. Also, synthesis of the RED is a complicated and laborious process. As an alternative to radioiodination, investigators labeled peptides with radiometals using chelating agents such as mercaptoacetyl-triglycerine, 2-iminothiolane, or a bifunctional metal-chelating peptide, but all of these chelating agents require complicated synthesis and are not readily available (11-13). Investigators have shown that EGF could be easily coupled to ^111^In via diethylenetriaminepentaacetic acid (DTPA), a readily available metal chelating agent, and used for in vitro studies with cultured cells (14, 15). The labeled EGF was internalized by the cells and translocated to the nucleus, and the radioactivity was shown to be bound to the chromatin. Orlova et al. reported that ^111^In conjugated to EGF, when internalized by the cells, had a superior cellular retention compared with ^125^I derived from directly radioiodinated EGF (16). In addition, ^111^In conjugated to EGF was reported to have a selective toxicity toward MDA-MB-468 cells, a human cancer cell line with high EGFR expression (15).

The use of radioactive yttrium (^90^Y, a high energy beta and Auger electrons emitter) conjugated to monoclonal Abs (MAbs) via DTPA was used to target human clonic tumors in nude mice, but the ^90^Y-DTPA complex was determined to be unstable, to accumulate in the liver, and to have a rapid blood clearance compared with the ^90^Y conjugate with the four isothiocyanatobenzyl (ITC-Bz) derivatives of DTPA (17). From this study the investigators concluded that the ITC-Bz derivatives of ^90^Y were superior to the DTPA conjugates. Because different Auger-emitting radiometals can be conjugated to peptides with DTPA and the DTPA-radiometal conjugates are not satisfactorily stable, Sundberg et al. decided to investigate the biological characteristics of ^111^In conjugated to benzyl-DTPA-human EGF(Bz-DTPA-hEGF) using the EGFR-rich U343MgaCl12:6 (U343) human glioma cell line under in vitro conditions (18). In another study, the biodistribution of ^111^In-DTPA-hEGF and ^111^In-Bz-DTPA-hEGF was compared in normal mice (19).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+Bz+DTPA+hEGF+synthesis)]

The synthesis of ^111^In-Bz-DTPA-hEGF was described by Sundberg et al. (18). Briefly, hEGF was obtained from commercial sources, and isothiocyanatebenzyl-DTPA (ITC-Bz-DTPA) was synthesized as described elsewhere (20). A hEGF solution in borate buffer (pH 9.1) was mixed with a solution of ITC-Bz-DTPA and left at room temperature overnight, and the Bz-DTPA-EGF conjugate was purified with reverse-phase high-performance liquid chromatography (RP-HPLC) with a SPEC C_18_ column using acetonitrile:water as the eluent. The buffer was then changed to acetate buffer (pH 6.5) using an NAP-5 column. The DTPA-hEGF conjugate was prepared and purified using procedures similar to those detailed above.

To obtain ^111^In-labeled hEGF, the radiometal was mixed with either DTPA-hEGF or Bz-DTPA-hEGF in ammonium acetate buffer (pH 6.0), and the mixtures were incubated at room temperature for 1 h (18). The labeled conjugates were purified with the use of a NAP-5 column, and the labeled products were eluted in phosphate-buffered saline (PBS). Analysis of the labeled products was performed with the use of a SPEC RP-HPLC C_18_ column.

Stability of the labeled hEGF conjugates was studied by mixing the PBS solutions of the labeled conjugates with calf serum and leaving the mixture at 37°C for 24 h. After incubation, analysis of the labeled products was performed with the use of a SPEC RP-HPLC C_18_ column.

The ^111^In labeling efficiency values for DTPA-hEGF and Bz-DTPA-hEGF were reported to be 89 ± 7% and 87 ± 4%, respectively (18). The radiochemical purity of the product was reported to be >96% as determined with RP-HPLC C_18_ column analysis. The maximum specific activity of the labeled peptides was reported to be 66 GBq/μmol (1.78 Ci/μmol). The serum stability of both conjugates was similar, and the transchelation of radioactivity to the blood proteins was reported to be 5.3% and 4.6% with ^111^In-Bz-DTPA-hEGF and ^111^In-DTPA-hEGF, respectively, at 37°C after 24 h.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111in+benzyl+dtpa+hegf+in+vitro)]

Sundberg et al. studied the binding and internalization of ^111^In-DTPA-hEGF and ^111^In-Bz-DTPA-hEGF with U343 cultured cells (18). The cells were exposed to the labeled peptides at 37°C for up to 24 h. The cells were harvested at different time points, washed with cold serum-free medium, and treated with ice-cold glycine buffer (pH 2.5) to remove any non-specific membrane or receptor-adhering radioactivity that has not been internalized. The cells were then treated with 1 M sodium hydroxide for at least 90 min and counted in a sodium iodide crystal to determine the amount of internalized radioactivity. Cellular internalization of both conjugates was reported to be rapid because the percent radioactivity within the cells was determined to be higher than the membrane-bound fraction (~45% versus ~10% for ^111^In-DTPA-hEGF, and ~60% versus ~15% for ^111^In-Bz-DTPA-hEGF at 8 h). To determine specificity of ^111^In-DTPA-hEGF and ^111^In-Bz-DTPA-hEGF binding, the cells were treated with the labeled conjugates in the presence of excess unlabeled EGF. Between the two conjugates, ^111^In-Bz-DTPA-hEGF was reported to have faster cell-binding kinetics. Presence of excess unlabled EGF almost eliminated the binding and internalization of both the labeled conjugates, indicating that the two labeled peptides had a high specificity for the EGFR.

Saturation studies with ^111^In-DTPA-hEGF and ^111^In-Bz-DTPA-hEGF showed that the U343 cells had a maximal binding (total number of receptors) of 0.09 pmol/10^5^ cells and a dissociation constant (K_d_) of 2.7 and 2.0 nM, respectively (18).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111in+benzyl+dtpa+hegf+rodentia)]

Tolmachev et al. compared the biodistribution of ^111^In-DTPA-hEGF and ^111^In-Bz-DTPA-hEGF in normal mice (19). The animals (n = 3/time point) were injected with the respective conjugates through the tail vein and euthanized at 0.5, 1, 4, and 24 h after injection. The blood and the main organs were then collected from the animals. Another set of animals (n = 3/labeled conjugate) were injected with 100 μg unlabeled hEGF, and the two labeled conjugates were respectively administered to the two groups of animals 0.5 h later. The animals were subsequently euthanized 0.5 h after administration of the labeled conjugates, and the various organs were collected as before. Radioactivity from both labeled conjugates was reported to clear rapidly from the blood with <1% remaining in circulation at 30 min. At any given time point, the amount of radioactivity remaining in circulation with ^111^In-Bz-DTPA-hEGF was two-fold that of ^111^In-DTPA-hEGF. Among the organs, radioactivity from both the labeled conjugates was detected primarily in the liver (~10 to 17.5% of the injected dose/g tissue (% ID/g)) and kidneys (~10 to 35% ID/g). In other organs, the accumulated radioactivity was ~0.5–3% ID/g with both labeled compounds. Treatment of the animals with unlabeled EGF followed by administration of the labeled conjugates resulted in a reduced accumulation of radioactivity in the liver, but an increased uptake of the label was observed in the kidneys during the same time. Also, an increased level of radioactivity was observed in the blood with both conjugates when the animals were pre-injected with unlabeled EGF. Compared with ^111^In-Bz-DTPA-hEGF, a significantly higher amount of ^111^In-DTPA-hEGF was reported to accumulate in the kidneys and bones of the animals. The area under the curve ratios for ^111^In-DTPA-hEGF versus ^111^In-Bz-DTPA-hEGF were determined to be 2.1 and 2.6 for the kidneys and bones, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+Bz+DTPA+hEGF+Non+Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+Bz+DTPA+hEGF+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+Bz+DTPA+hEGF+Human+Studies)]

No references are currently available.

## References

1 Belda-Iniesta C., de Castro Carpeno J., Sereno M., Gonzalez-Baron M., Perona R. (2008). Epidermal growth factor receptor and glioblastoma multiforme: molecular basis for a new approach. Clin Transl Oncol.
2 Normanno N., De Luca A., Bianco C., Strizzi L., Mancino M., Maiello M.R., Carotenuto A., De Feo G., Caponigro F., Salomon D.S. (2006). Epidermal growth factor receptor (EGFR) signaling in cancer. Gene.
3 Burgess A.W. (2008). EGFR family: structure physiology signalling and therapeutic targets. Growth Factors.
4 Wang Q., Villeneuve G., Wang Z. (2005). Control of epidermal growth factor receptor endocytosis by receptor dimerization, rather than receptor kinase activation. EMBO Rep.
5 Ogawa M., Regino C.A., Choyke P.L., Kobayashi H. (2009). In vivo target-specific activatable near-infrared optical labeling of humanized monoclonal antibodies. Mol Cancer Ther.
6 Lewis Phillips G.D., Li G., Dugger D.L., Crocker L.M., Parsons K.L., Mai E., Blattler W.A., Lambert J.M., Chari R.V., Lutz R.J., Wong W.L., Jacobson F.S., Koeppen H., Schwall R.H., Kenkare-Mitra S.R., Spencer S.D., Sliwkowski M.X. (2008). Targeting HER2-positive breast cancer with trastuzumab-DM1, an antibody-cytotoxic drug conjugate. Cancer Res.
7 Dahle J., Borrebaek J., Jonasdottir T.J., Hjelmerud A.K., Melhus K.B., Bruland O.S., Press O.W., Larsen R.H. (2007). Targeted cancer therapy with a novel low-dose rate alpha-emitting radioimmunoconjugate. Blood.
8 Dadparvar S. Krishna L. Miyamoto C. Brady L.W. Brown S.J. Bender H. Slizofski W.J. Eshleman J. Chevres A. Woo D.V. Indium-111-labeled anti-EGFr-425 scintigraphy in the detection of malignant gliomas Cancer 1994 73Suppl3 884 9 8306274
9 Blomquist E., Carlsson J. (1992). Strategy for planned radiotherapy of malignant gliomas: postoperative treatment with combinations of high dose proton irradiation and tumor seeking radionuclides. Int J Radiat Oncol Biol Phys.
10 Lindstrom A., Carlsson J. (1993). Penetration and binding of epidermal growth factor-dextran conjugates in spheroids of human glioma origin. Cancer Biother.
11 Capala J., Barth R.F., Bailey M.Q., Fenstermaker R.A., Marek M.J., Rhodes B.A. (1997). Radiolabeling of epidermal growth factor with 99mTc and in vivo localization following intracerebral injection into normal and glioma-bearing rats. Bioconjug Chem.
12 Hnatowich D.J., Qu T., Chang F., Ley A.C., Ladner R.C., Rusckowski M. (1998). Labeling peptides with technetium-99m using a bifunctional chelator of a N-hydroxysuccinimide ester of mercaptoacetyltriglycine. J Nucl Med.
13 Remy S., Reilly R.M., Sheldon K., Gariepy J. (1995). A new radioligand for the epidermal growth factor receptor: 111In labeled human epidermal growth factor derivatized with a bifunctional metal-chelating peptide. Bioconjug Chem.
14 Reilly R.M., Gariepy J. (1998). Factors influencing the sensitivity of tumor imaging with a receptor-binding radiopharmaceutical. J Nucl Med.
15 Reilly R.M., Kiarash R., Cameron R.G., Porlier N., Sandhu J., Hill R.P., Vallis K., Hendler A., Gariepy J. (2000). 111In-labeled EGF is selectively radiotoxic to human breast cancer cells overexpressing EGFR. J Nucl Med.
16 Orlova A., Bruskin A., Sjostrom A., Lundqvist H., Gedda L., Tolmachev V. (2000). Cellular processing of (125)I- and (111)in-labeled epidermal growth factor (EGF) bound to cultured A431 tumor cells. Nucl Med Biol.
17 Sharkey R.M., Motta-Hennessy C., Gansow O.A., Brechbiel M.W., Fand I., Griffiths G.L., Jones A.L., Goldenberg D.M. (1990). Selection of a DTPA chelate conjugate for monoclonal antibody targeting to a human colonic tumor in nude mice. Int J Cancer.
18 Sundberg A.L., Orlova A., Bruskin A., Gedda L., Carlsson J., Blomquist E., Lundqvist H., Tolmachev V. (2003). [(111)In]Bz-DTPA-hEGF: Preparation and in vitro characterization of a potential anti-glioblastoma targeting agent. Cancer Biother Radiopharm.
19 Tolmachev V., Orlova A., Wei Q., Bruskin A., Carlsson J., Gedda L. (2004). Comparative biodistribution of potential anti-glioblastoma conjugates [111In]DTPA-hEGF and [111In]Bz-DTPA-hEGF in normal mice. Cancer Biother Radiopharm.
20 Williams A., Rapoport H. (1993). Synthesis of enantiomerically pure diethylenetriamine pentaacetic acid analogues:L-phenylalanine as the educt for substitution at the central acetic acid. J. Org. Chem.